# Bismuth sulphide polyvinylpyrrolidone nanoparticles

Chemical name: | Bismuth sulphide polyvinylpyrrolidone nanoparticles
Abbreviated name: | BPNPs
Synonym: | Bi_2_S_3_ PVP nanoparticles
Agent Category: | Metal
Target: | Phagocytes
Target Category: | Phagocytosis, endocytosis
Method of detection: | X-ray, CT
Source of signal: | Bi
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles)]

X-ray imaging, or computed tomography (CT), visualizes tissue density differences that provide the image contrast produced by X-ray attenuation between soft tissues and electron-dense bone (1). Contrast enhancement with the use of X-ray contrast (radiopaque) agents are needed to increase the degree of contrast between diseased tissues and normal tissues. Water-soluble X-ray contrast agents are generally based on small tri-iodobenzene compounds such as monomers or dimers (2), which can be ionic (high osmolality) or nonionic (low osmolality). When injected intravenously, commonly via intra-arterial catheterization, these agents exhibit highly nonspecific vascular permeation and rapid renal excretion, which limits their targeting performance.

Bismuth salts were used as X-ray contrast agents in the gastrointestinal tract as early as 1897 (1). However, their use did not continue because high doses of bismuth salts are toxic. Rabin et al. (3) have performed experiments using polyvinylpyrrolidone (PVP)-coated Bi_2_S_3_ nanoparticles (BPNPs) as a CT contrast agent. This preparation exhibited excellent stability, high X-ray absorption (5-fold better than iodine provided as iopromide), a good efficacy/safety profile, long blood half-life, and enhanced CT contrast of the vasculature, liver, and lymph nodes in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20synthesis)]

Rabin et al. (3) reported that Bi_2_S_3_ nanocrystals were grown by precipitation of bismuth citrate and sodium sulphide in the presence of 3-mercaptopropionic acid. The reaction mixture was then filtered and lyophilized. The nanocrystals were resuspended in aqueous PVP and dialyzed against aqueous polyethylene oxide. The mean hydrodynamic diameter of the BPNPs as measured by laser-light scattering was 30 ± 10 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20in%20vitro)]

X-ray fluoroscopic study showed that a 0.55 M in bismuth concentration of BPNPs solution was equivalent in X-ray absorption to a 2.36-M iodine solution of iopromide (3). Cytotoxicity studies of BPNPs and bismuth subsalicylate using U937 human macrophages and HepG2 hepatocytes showed that bismuth subsalicylate had lethal dose (LD_50_) values of 8 and 5 mM, respectively. On the other hand, bismuth from BPNPs had LD_50_ values of 100 and 114 mM, respectively. Therefore, bismuth provided via BPNPs was >10-fold less toxic to cells than bismuth provided via bismuth subsalicylate. BPNPs also exhibited a better efficacy/toxicity ratio than iopromide in hepatocytes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20rodentia)]

In mice, BPNPs (57 μmol bismuth-equivalent/mouse) had a half-life of 140 ± 15 min in blood after intravenous injection as compared to <10 min for commercial iodinated preparations (3). CT imaging up to 48 h showed clear delineation of the cardiac ventricles, all major blood vessels, and the liver at 24 h. Weak contrast was visualized in the kidneys and urinary tract at 24–48 h. No residual bismuth was detected in any organ in the mice 2 months after the injection of BPNPs. Regional lymph nodes were clearly delineated up to 140 h after subcutaneous injection of BPNPs (11.4 μmol bismuth-equivalent). The authors suggested that further biodistribution and histological studies are required to fully assess the safety and usefulness of BPNPs as a CT agent in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Bismuth%20sulphide%20nanoparticles%20and%20human)]

No publication is currently available.

## NIH Support

P50 CA86355, R24 CA92782, UO1 HL080731, U54 CA119349, RO1-EB004626A01

## References

1 Yu S.B., Watson A.D. (1999). Metal-based X-ray contrast media. Chem Rev.
2 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
3 Rabin O., Manuel Perez J., Grimm J., Wojtkiewicz G., Weissleder R. (2006). An x-ray computed tomography imaging agent based on long-circulating bismuth sulphide nanoparticles. Nat Mater.